# Cy5-Tat-Glu-Pro-Asp-acyloxymethyl ketone

Chemical name: | Cy5-Tat-Glu-Pro-Asp-acyloxymethyl ketone
Abbreviated name: | tAB50-Cy5
Synonym:
Agent Category: | Small molecule
Target: | Caspase-3, caspase-7
Target Category: | Enzyme
Method of detection: | Optical, near-infrared fluorescence imaging
Source of signal / contrast: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=apoptosis+and+molecular+imaging)]

Caspases are a group of cysteine proteases, which exist within cells as inactive zymogens, and are cleaved to form active enzymes after induction of apoptosis (1-3). There are two major pathways through which caspases are activated. One is the death signal–induced, death receptor–mediated extrinsic pathway, and the other is the stress-induced, mitochondria-directed intrinsic pathway (3, 4). Caspases convey the apoptotic signal in a proteolytic cascade, with caspases cleaving and activating other caspases. Caspase-8 and -9 act as initiators at the upper stream of this cascade, while caspase-3, -6, and -7 work as downstream executioners (1, 3, 4). Although physiological apoptosis takes place during embryonic development and in adult homeostasis, excessive apoptosis has been observed in some human diseases such as myocardial infarction, rheumatoid arthritis, ischemia, transplant rejection, and neurodegenerative disorders (Parkinson's and Alzheimer's) (5, 6). On the contrary, evading apoptosis is a hallmark of human cancer (7, 8).

Many different molecular probes have been developed for imaging apoptosis both at the cellular level and in vivo (2, 5, 7, 9, 10). Of them, a large number of the probes are annexin V–based. Annexin V is a 36-kDa protein that binds to externalized phosphatidylserine residues in the presence of calcium ions on the surface of apoptotic cells (5). Radiolabeled annexin V derivatives have already been used for clinical imaging in many diseases, most notably for imaging myocardial dysfunction. A drawback of annexin V–based probes is their low specificity to apoptotic cells. Annexin V cannot distinguish apoptosis from necrosis (5). Phosphatidylserine externalization is also associated with inflammation and platelet activation, causing further challenges with annexin V specificity. During recent years, much work has focused on the development of probes for caspase-3 and -7. Thornberry et al. have observed that most caspases prefer a tetrapeptide motif with an aspartyl residue at P4 (11). Asp-Glu-Val-Asp (DEVD) is the peptide sequence optimal for caspase-3 and -7, while the Val-Glu-His-Asp (VEHD) sequence is preferred by caspase-6 (5). These sequence-based probes demonstrate high caspase specificity; however, most probes suffer from poor cellular uptake in the intact cell, a requirement for early detection.

Edgington et al. developed a class of probes based on the acyloxymethyl ketone (AOMK) and the optimal sequence of caspase-3 and -7 (2). AB50-Cy5 is one of the probes, which contains a Glu-Pro-Asp-AOMK sequence labeled with the Cy5 fluorophore. This probe showed labeling of caspase-3 and legumain with no detectable cathepsin B labeling. To enhance the cell permeability of AB50-Cy5, the investigators synthesized the probe tAB50-Cy5, a version of the probe containing a tat peptide. For this probe, the tat peptide was used to increase the cell uptake of the probe through multiple positively charged amino acids, while AOMK was used to label caspases. This chapter summarized the synthesis and comparative analysis of tAB50-Cy5 and AB50-Cy5.

### Related Resource Links:

- Chapter of AB50-Cy5 (or Cy5-AB50) in MICAD (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=AB50_Cy5)
- Apoptosis imaging chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=apoptosis+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Apoptosis related information in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=apoptosis)
- Apoptosis imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=apoptosis+and+molecular+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19597506)]

The detailed synthesis of AB50-Cy5 and tAB50-Cy5 was described by Edgington et al. and can also be found in the MICAD chapter for AB50-Cy5 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=AB50_Cy5) (2). The tat version, tAB50-Cy5, differed from AB50-Cy5 in that the Cy5 fluorochrome was moved to a lysine side chain, and the tat peptide was coupled through a cysteine residue to a maleimide group at the amino terminus of the probe. The tat peptide (Arg-Lys-Lys-Arg-Arg-Orn-Arg-Arg-Arg-Cys, all D-amino acids, except for the cysteine) was custom synthesized. Edgington et al. also generated the control version of tAB50-Cy5 (tAB50-Ctrl) that contains an amide in place of the reactive AOMK functional group. The purity and identity of all probes were assessed with liquid chromatography-mass spectrometry analysis (detailed data not shown).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19597506)]

Edgington et al. used SDS-PAGE gel analysis to evaluate the probes' ability to label caspases (2). As expected, the active probes AB50-Cy5 and tAB50-Cy5 efficiently labeled recombinant caspase-3, whereas control probes did not. In intact Jurkat cells, when the cells were first treated with anti-Fas antibody to activate apoptosis and then labeled with probes, both AB50-Cy5 and tAB50-Cy5 labeled caspases. When the cells were pretreated with the probes, followed by washout before apoptosis activation with anti-Fas antibody, only tAB50-Cy5 showed labeling of caspases. These results indicated that the tat peptide increased the penetrating ability of the probes into intact cells. However, addition of the tat peptide also resulted in a substantial increase in the labeling of legumain (MICAD chapter for AB50-Cy5 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=AB50_Cy5)). This increase in labeling of a lysosome-resident protease is probably due to uptake of the probes via the endo-lysosomal route before release into the cytosol.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19597506)]

To test the utility of tAB50-Cy5 for imaging apoptosis, Edgington et al. monitored caspase activation in mice treated with dexamethasone for 6, 12, or 24 h (n = 3 mice for each time point) (2). Probes were injected intravenously 2 h before removal of thymi for imaging and SDS-PAGE analysis. The results showed that AB50-Cy5 and tAB50-Cy5 had same trend in fluorescent signals in the intact thymi and the same pattern in labeling caspases and legumain (labeled both caspase-3 and legumain), but the overall signal intensity increased for tAB50-Cy5. The amount of labeled caspases directly correlated with the imaging signal intensity. A similar increase in tAB50-Cy5 signal was not observed in the samples treated with vehicle, suggesting increased uptake of the probe only into apoptotic cells. Quantitative analysis revealed that legumain activity was low and remained largely unchanged in the first 12 h after dexamethasone treatment. Different from legumain, caspase-3 activity was observable at 6 h after treatment, peaking at 12 h and then sharply dropping to background levels at 24 h after injection. These data agreed with previous studies that showed a peak in TUNEL^+^ thymocyte staining at 16 h after dexamethasone treatment followed by a sharp decrease at 18 h and 24 h. Flow cytometry further confirmed that tAB50-Cy5 accumulated only in dying cells, and the probe-positive cells were also positive for annexin V. These results suggested that caspases are likely to be activated at early time points and, therefore, may serve as effective markers of the early stages of apoptosis. The fluorescence observed in whole organs can be used as a direct readout of total probe-labeled proteases.

Edgington et al. further monitored caspase activation in xenografted human tumor tissues that had been induced to undergo apoptosis by treatment with the monoclonal antibody Apomab (2). Apomab induces the extrinsic apoptosis pathway by binding death receptor-5 and is highly distinct from the dexamethasone-induced intrinsic apoptosis in CD4^+^CD8^+^ thymocytes. In agreement with the results obtained for the dexamethasone model, total fluorescent signals in the tumors closely mirrored levels of labeled caspase-3 and -7. The maximum caspase activity occurred 12 h after Apomab treatment, while the overall levels of legumain labeling were constant throughout the time course. tAB50-Cy5 showed substantially brighter signals but had slow clearance from all tissues, resulting in a low signal/background ratio at the early time points with optimal contrast (4.5-fold) at 5 h after probe injection. AB50-Cy5, in contrast, cleared rapidly and showed a good signal/background ratio even at the early time points (3.2-fold contrast at 50 min). Notably, tAB50-Ctrl showed nearly identical accumulation in Apomab-treated tumors as tAB50-Cy5 but also produced higher background fluorescence in vehicle-treated tumors. Thus, although the control probes had some accumulation in apoptotic cells, only the active probes showed a marked contrast between apoptotic and nonapoptotic tumors. The ex vivo images closely matched the images obtained in live mice. Specific labeling of caspases was observed only in Apomab-treated samples. Specific labeling of apoptotic cells was further confirmed with histology of tumor tissues.

The investigators concluded that caspase-specific probes can be used to noninvasively monitor apoptosis in tumors treated with chemotherapy agents (2). The non–tat-labeled probes provide the best direct readout of caspase activity, but the tat-labeled probes boost overall specific signal and may therefore be useful for carrying other contrast agents into apoptotic cells. The cross-reactivity with legumain does not appear to hinder the probes' ability to monitor dynamic changes in caspase activity because of the constant low activity of legumain during apoptosis.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Fan T.J., Han L.H., Cong R.S., Liang J. (2005). Caspase family proteases and apoptosis. Acta Biochim Biophys Sin (Shanghai).
2 Edgington L.E., Berger A.B., Blum G., Albrow V.E., Paulick M.G., Lineberry N., Bogyo M. (2009). Noninvasive optical imaging of apoptosis by caspase-targeted activity-based probes. Nat Med.
3 Salvesen G.S., Riedl S.J. (2008). Caspase mechanisms. Adv Exp Med Biol.
4 Boatright K.M., Salvesen G.S. (2003). Mechanisms of caspase activation. Curr Opin Cell Biol.
5 Smith G., Nguyen Q.D., Aboagye E.O. (2009). Translational imaging of apoptosis. Anticancer Agents Med Chem.
6 Shirvan A., Reshef A., Yogev-Falach M., Ziv I. (2009). Molecular imaging of neurodegeneration by a novel cross-disease biomarker. Exp Neurol.
7 Nguyen Q.D., Smith G., Glaser M., Perumal M., Arstad E., Aboagye E.O. (2009). Positron emission tomography imaging of drug-induced tumor apoptosis with a caspase-3/7 specific [18F]-labeled isatin sulfonamide. Proc Natl Acad Sci U S A.
8 Ledgerwood E.C., Morison I.M. (2009). Targeting the apoptosome for cancer therapy. Clin Cancer Res.
9 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
10 Paulick M.G., Bogyo M. (2008). Application of activity-based probes to the study of enzymes involved in cancer progression. Curr Opin Genet Dev.
11 Thornberry N.A., Rano T.A., Peterson E.P., Rasper D.M., Timkey T., Garcia-Calvo M., Houtzager V.M., Nordstrom P.A., Roy S., Vaillancourt J.P., Chapman K.T., Nicholson D.W. (1997). A combinatorial approach defines specificities of members of the caspase family and granzyme B. Functional relationships established for key mediators of apoptosis. J Biol Chem.